# R-2-[^131^I]Iodophenyl-(1-(1-methylpiperidin-2-ylmethyl)-1H-indol-3-yl)methanone

Chemical name: | R-2-[^131^I]Iodophenyl-(1-(1-methylpiperidin-2-ylmethyl)-1H-indol-3-yl)methanone
Abbreviated name: | R-[^131^I]AM2233
Synonym:
Agent Category: | Compound
Target: | Cannabinoid CB1receptors
Target Category: | Receptor binding
Method of detection: | SPECT, gamma planar
Source of signal: | ^131^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AM2233%20and%20131I)]

There are two subtypes of cannabinoid receptors in mammalian tissues: CB1 and CB2 (1, 2). CB1 receptors are expressed abundantly in neuronal terminals in the central nervous system (CNS) and peripheral tissues to inhibit neurotransmitter release. CB1 receptors are found predominantly in the striatum, hippocampus, substantia nigra, globus pallidus, and cerebellum. CB2 receptors are present mainly on immune cells to modulate cytokine release. Both receptor subtypes are coupled through G_i/o_ proteins to inhibit adenylate cyclase and to modulate potassium and calcium channels. CB1 receptors have been demonstrated to be involved in analgesia, regulation of food intake, and control of movement in normal subjects (3). Alteration of CB1 receptor function has been implicated in a number of human diseases such as depression, schizophrenia, and obesity (4-6).

Δ9-Tetrahydrocannabinol (THC) is a major active cannabinoid that is found in marijuana and activates CB1 receptors (7). However, high lipophilicity is essential for binding to CB1 receptors, and moderate lipophilicity is required for crossing the blood–brain barrier (BBB). Existing radiolabeled ligands are mainly analogs of the antagonist rimonabant (SR141716A) and the agonist WIN 55,212-2; however, these ligands also exhibit high nonspecific binding, which limits their application in imaging (8). R-2-Iodophenyl-(1-(1-methylpiperidin-2-ylmethyl)-1H-indol-3-yl)methanone (R-AM2233) is a potent CB agonist with ~8-fold higher affinity than WIN 55,212-2 (9). R-2-[^131^I]Iodophenyl-(1-(1-methylpiperidin-2-ylmethyl)-1H-indol-3-yl)methanone (R- [^131^I]AM2233) is being developed as a single photon emission computed tomography agent for the noninvasive study of CB1 receptors in the brain (9, 10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AM2233%20and%20131I%20and%20synthesis)]

Deng et al. (9) reported synthesis of R-[^131^I]AM2233 by radioiododestannylation of the tributyltin precursor R-[1-(1-methylpiperidin-2-ylmethyl)-1H-indol-3-yl]-2-(tributylstannylphenyl)methanone with ^131^I-labeled iodide in the presence of HCl and chloramine-T. Radiochemical yields were 62% after high-performance liquid chromatography purification. Specific activities were >18.5 GBq/μmol (>0.5 Ci/μmol) with a radiochemical purity of >97%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AM2233%20and%20131I%20and%20in%20vitro)]

Deng et al. (9) reported R/S-AM2233 had an inhibitory constant (K_i_) value of 2.8 nM for CB1 receptors in rat forebrain membranes and a K_i_ value of 2.9 nM for CB2 receptors in mouse spleen membranes. The R-enantiomer is 300-fold more potent than the S-enantiomer. R/S-AM2233 and WIN 55,212-2 exhibited K_i_ values of 0.2 and 1.6 nM in displacing R-[^131^I]AM2233 in mouse hippocampus membranes. R/S-AM2233 and WIN 55,212-2 exhibited K_i_ values of 1.3 and 20 nM in displacing [^3^H]SR141716 in mouse hippocampus membranes. Therefore, R/S-AM2233 is 8- to 15-fold more potent than WIN 55,212-2. In vitro autoradiography of mouse brain sections showed that R-[^131^I]AM2233 gave images consistent with binding to brain CB1 receptor-rich areas, including the globus pallidus, substantia nigra, striatum, cerebellum, and hippocampus. Binding of S-[^131^I]AM2233 in these brain sections was much reduced compared with that of R/S-[^131^I]AM2233. Selective binding of R-[^131^I]AM2233 was not detected in sections prepared from a CB1 receptor knockout mouse, confirming that in vitro binding was caused by CB1 receptors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AM2233%20and%20131I%20and%20rodentia)]

Dhawan et al. (10) showed there was a low uptake of radioactivity in the mouse whole brain after injection of R-[^131^I]AM2233, reaching a peak value of 1.3% injected dose per gram (% ID/g) at 5 min and declining to 0.6% ID/g at 30 min. The hippocampus exhibited higher uptake than the cerebellum, brain stem, and whole brain. Co-injection of 3 mg/kg of SR141716A with R-[^131^I]AM2233 reduced the radioactivity to nonspecific levels in the striatum, globus pallidus, and substantia nigra. However, the hippocampus exhibited only 69% reduction because of tentative binding to non-CB1 receptors in the region. Co-injection of 10 mg/Kg WIN 55,212-2 reduced R-[^131^I]AM2233 specific binding in CB1 receptor-rich areas by only 21–43%. Ex vivo autoradiography of rat brain showed the high levels of radioactivity in the substantia nigra, globus pallidus, hippocampus, and cerebellum, followed by the cortex, striatum, and thalamus at 15–30 min after R-[^131^I]AM2233 injection, consistent with the CB1 distribution in the brain.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AM2233%20and%20131I%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AM2233%20and%20131I%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AM2233%20and%20131I%20and%20human)]

No publication is currently available.

## NIH Support

DA-112-01, DA-3801, DA-12412, DA-3801, DA-9158

## References

1 Howlett A.C., Barth F., Bonner T.I., Cabral G., Casellas P., Devane W.A., Felder C.C., Herkenham M., Mackie K., Martin B.R., Mechoulam R., Pertwee R.G. (2002). International Union of Pharmacology. XXVII. Classification of cannabinoid receptors. Pharmacol Rev.
2 Pertwee R.G. (1997). Pharmacology of cannabinoid CB1 and CB2 receptors. Pharmacol Ther.
3 Pertwee R.G. (2005). Pharmacological actions of cannabinoids. Handb Exp Pharmacol, (168): p. 1-51.
4 Gambi F., De Berardis D., Sepede G., Quartesan R., Calcagni E., Salerno R.M., Conti C.M., Ferro F.M. (2005). Cannabinoid receptors and their relationships with neuropsychiatric disorders. Int J Immunopathol Pharmacol.
5 De Vries T.J., Schoffelmeer A.N. (2005). Cannabinoid CB1 receptors control conditioned drug seeking. Trends Pharmacol Sci.
6 Guzman M., Sanchez C. (1999). Effects of cannabinoids on energy metabolism. Life Sci.
7 Martin B.R. (1986). Cellular effects of cannabinoids. Pharmacol Rev.
8 Gifford A.N., Makriyannis A., Volkow N.D., Gatley S.J. (2002). In vivo imaging of the brain cannabinoid receptor. Chem Phys Lipids.
9 Deng H., Gifford A.N., Zvonok A.M., Cui G., Li X., Fan P., Deschamps J.R., Flippen-Anderson J.L., Gatley S.J., Makriyannis A. (2005). Potent cannabinergic indole analogues as radioiodinatable brain imaging agents for the CB1 cannabinoid receptor. J Med Chem.
10 Dhawan J., Deng H., Gatley S.J., Makriyannis A., Akinfeleye T., Bruneus M., Dimaio A.A., Gifford A.N. (2006). Evaluation of the in vivo receptor occupancy for the behavioral effects of cannabinoids using a radiolabeled cannabinoid receptor agonist, R-[125/131I]AM2233. Synapse.